# ^89^Zr-Desferrioxamine p-isothiocyanatobenzyl-anti-hepatocyte growth factor receptor 1-armed antibody onartuzumab

Chemical name: | ^89^Zr-Desferrioxamine p-isothiocyanatobenzyl-anti-hepatocyte growth factor receptor 1-armed antibody onartuzumab
Abbreviated name: | 89Zr-Df-Onartuzumab
Synonym:
Agent category: | Antibody fragment, 1-armed antibody
Target: | Hepatocyte growth factor receptor (HGFR, MET)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/AAA64297.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_000601.4) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/gene/3082) for more information about HGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Onartuzumab)]

MET is a proto-oncogene protein, also known as c-Met or hepatocyte growth factor (HGF) receptor (HGFR) (1). MET is a membrane receptor with tyrosine kinase activity that is essential for embryonic development and wound healing. MET is normally expressed by stem cells, progenitor cells, and cells of epithelial origin, whereas expression of HGF, which is the only known ligand of MET, is restricted to cells of mesenchymal origin. Upon HGF stimulation, MET induces several biological responses that lead to invasive growth (2). Abnormal MET activation in cancer correlates with poor prognosis because deregulated MET triggers tumor growth, induces angiogenesis, and activates metastasis (3). MET and HGF are overexpressed in many types of human malignancies, including kidney, liver, stomach, breast, and brain cancers (2, 4, 5). Inhibition of MET function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (6). On the other hand, targeting HGF instead of the HGF receptor may also be beneficial to patients by blocking binding of HGF to MET.

Monoclonal antibody DN30 (150 kDa) is directed against the extracellular domain of MET, with a K_d_ of 2.64 nM (6). Inhibition of HGFR function with DN30 has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis. Perk et al. (7) prepared ^89^Zr-N-succinyldesferrioxamine-DN30 (^89^Zr-DN30) for imaging MET expression in tumors, showing tumor accumulation corresponding to MET expression levels. However, DN30 is a partial agonist with partial biological responses. Onartuzumab is a MET-selective humanized 1-armed monoclonal antibody (100 kDa) with anti-proliferation, anti-angiogenic, and pro-apoptotic properties against tumor growth in mouse tumor models (8). Onartuzumab is a pure antagonist with monovalent binding to MET. For use with positron emission tomography (PET), onartuzumab was conjugated with the bifunctional chelate p-isothiocyanatobenzyl-desferrioxamine (Df-Bz-NCS) and labeled with ^89^Zr to form ^89^Zr-Df-onartuzumab for imaging MET expression in tumors (9).

### Related Resource Links:

- Chapters in MICAD (HGF (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=HGF+AND+micad%5Bbook%5D), c-Met (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=c-Met+AND+micad%5Bbook%5D))
- Gene information in NCBI (HGF (http://www.ncbi.nlm.nih.gov/gene/3082), c-Met (http://www.ncbi.nlm.nih.gov/gene/4233))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HGF (http://omim.org/entry/142409), c-Met (http://omim.org/entry/164860))
- Clinical trials (HGF (http://www.clinicaltrials.gov/ct2/results?term=hepatocyte+growth+factor), c-Met (http://www.clinicaltrials.gov/ct2/results?term=c-Met), onartuzumab (http://www.clinicaltrials.gov/ct2/results?term=Onartuzumab&Search=Search))
- Drug information in FDA (c-Met (http://google2.fda.gov/search?q=c-Met&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Onartuzumab+synthesis)]

Df-Onartuzumab was prepared by incubation of onartuzumab with Df-Bz-NCS in buffer (pH 9) for 30 min at 37°C (9). Df-Onartuzumab was purified with column chromatography. The number of Df groups per onartuzumab was not reported. For ^89^Zr-labeling, a solution of 74–148 MBq (2–4 mCi) ^89^Zr in 1 M oxalic acid and Df-onartuzumab was incubated in HEPES buffer (pH 7.0) for 60 min at room temperature. The labeling yields were >90%. The specific activities of ^89^Zr-Df-onartuzumab were 37–185 MBq/nmol (1–5 mCi/nmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Onartuzumab+in+vitro)]

In cell-based saturation assays with human gastric cancer MKN-45 cells, ^89^Zr-Df-onartuzumab exhibited an affinity constant (K_d_) value of 6.12 ± 1.18 nM (n = 3) and a B_max_ value of 0.94 ± 0.08 × 10^6^ sites/cell (n = 3) (9). The immunoreactivity of ^89^Zr-Df-onartuzumab was 81.9 ± 0.7% (n = 3).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Onartuzumab+rodentia)]

Jagoda et al. (9) performed ex vivo biodistribution studies of 1.85 MBq (0.05 mCi) ^89^Zr-Df-onartuzumab (~0.5 nmol) in nude mice bearing MKN-45 tumors (high MET expression) or U87MG tumors (low MET expression) (n = 4–5 mice/group) at 1, 2, 3, 4, and 5 d after injection. Accumulation in MKN-45 tumors was 10% injected dose/gram (ID/g) at 1 d and gradually increased to 23% ID/g at 5 d. Accumulation in the non-targeted tissues (blood, heart, lung, gastrointestinal tract, and muscle) decreased slowly, with ~50% reduction from 1 d to 5 d. On the other hand, radioactivity in the liver and kidney increased with time, suggesting hepatobiliary and renal clearance. Accumulation in the tumors was higher than in all other tissues at 2–5 d. Accumulation in U87MG tumors was 1.8- and 3.0-fold lower than that in the MKN-45 tumors at 3 d and 5 d, respectively. The tumor/muscle ratios for MKN-45 tumors were 13.2, 26.5, and 26.6 at 2, 3, and 5 d, respectively. On the other hand, the tumor/muscle ratios for U87MG tumors were 7 and 9 at 2 d and 5 d, respectively. Co-injection of excess onartuzumab (10 nmol/mouse) was performed with mice bearing MKN-45 tumors (n = 4 mice) with 0.37 MBq (0.01 mCi) ^89^Zr-Df-onartuzumab (~0.03 nmol) at 3 d after injection. Tumor accumulation was reduced by 67%.

Whole-body PET imaging studies were performed in mice bearing MKN-45 xenografts at 1–5 d after injection of 7.4 MBq (0.2 mCi) ^89^Zr-Df-onartuzumab (1.2 nmol) (9). The tumors could be visualized at 1 d with improving quality over the 5-d period. The tumor/muscle ratio was 26 at 5 d.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Onartuzumab+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Onartuzumab+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Onartuzumab+human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Boccaccio C., Comoglio P.M. (2006). Invasive growth: a MET-driven genetic programme for cancer and stem cells. Nat Rev Cancer.
2 Di Renzo M.F., Olivero M., Giacomini A., Porte H., Chastre E., Mirossay L., Nordlinger B., Bretti S., Bottardi S., Giordano S., et al. (1995). Overexpression and amplification of the met/HGF receptor gene during the progression of colorectal cancer. Clin Cancer Res.
3 Lengyel E., Prechtel D., Resau J.H., Gauger K., Welk A., Lindemann K., Salanti G., Richter T., Knudsen B., Vande Woude G.F., Harbeck N. (2005). C-Met overexpression in node-positive breast cancer identifies patients with poor clinical outcome independent of Her2/neu. Int J Cancer.
4 Smith H.S., Stern R., Liu E., Benz C. (1991). Early and late events in the development of human breast cancer. Basic Life Sci.
5 Di Renzo M.F., Olivero M., Serini G., Orlandi F., Pilotti S., Belfiore A., Costantino A., Vigneri R., Angeli A., Pierotti M.A., et al. (1995). Overexpression of the c-MET/HGF receptor in human thyroid carcinomas derived from the follicular epithelium. J Endocrinol Invest.
6 Petrelli A., Circosta P., Granziero L., Mazzone M., Pisacane A., Fenoglio S., Comoglio P.M., Giordano S. (2006). Ab-induced ectodomain shedding mediates hepatocyte growth factor receptor down-regulation and hampers biological activity. Proc Natl Acad Sci U S A.
7 Perk L.R., Stigter-van Walsum M., Visser G.W., Kloet R.W., Vosjan M.J., Leemans C.R., Giaccone G., Albano R., Comoglio P.M., van Dongen G.A. (2008). Quantitative PET imaging of Met-expressing human cancer xenografts with (89)Zr-labelled monoclonal antibody DN30. Eur J Nucl Med Mol Imaging.
8 Martens T., Schmidt N.O., Eckerich C., Fillbrandt R., Merchant M., Schwall R., Westphal M., Lamszus K. (2006). A novel one-armed anti-c-Met antibody inhibits glioblastoma growth in vivo. Clin Cancer Res.
9 Jagoda E.M., Lang L., Bhadrasetty V., Histed S., Williams M., Kramer-Marek G., Mena E., Rosenblum L., Marik J., Tinianow J.N., Merchant M., Szajek L., Paik C., Cecchi F., Raffensperger K., Jose-Dizon J.M., Bottaro D.P., Choyke P. (2012). Immuno-PET of the Hepatocyte Growth Factor Receptor Met Using the 1-Armed Antibody Onartuzumab. J Nucl Med.